# Green fluorescent protein specified small interfering RNA-cross-linked iron oxide nanoparticles-Cy5.5

Chemical name: | Green fluorescent protein specified small interfering RNA –crosslinked iron oxide nanoparticles-Cy5.5
Abbreviated name: | siGFP-CLIO-Cy5.5
Synonym: | MN-NIFR-siGFP
Agent category: | Nucleic acid, small molecule (nanoparticle)
Target: | RNAse III
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI), near-infrared (NIFR) optical imaging
Source of signal/contrast: | Iron oxides, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is Currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLIO + cy5.5 + siGFP)]

Ribonucleic acid interference (RNAi) modulates intracellular activation via the use of small interfering RNA (siRNA) (1). RNAi suppresses gene expression through degradation of a specific, targeted mRNA, which leads to gene silencing. siRNA is a 21-23 nucleotide (nt) double-stranded RNA (dsRNA) with symmetric 2-3nt 3’ overhangs and 5’-phosphate and 3’-hydroxyl groups so that it is recognized by an RNAse III enzyme (2). In general, intracellular siRNA undergoes 5’-phosphorylation to unwind the RNA duplex, followed by association with RNA-induced silencing complex (RISC) (1). Then the activated RISC and the unwound anti-sense strand of the siRNA interact with the mRNA target to generate single site-specific cleavage at the mRNA target. The efficiency of gene silencing primarily relies on the optimal incorporation of siRNA into RISC and its stability in RISC, as well as a perfect complementary base pairing with the mRNA target (3). Mismatches can abolish the target degradation, the mRNA cleavage, and the RISC turnover. The high specificity in gene silencing makes siRNA a popular research tool for various gene-inactivation studies such as differentiation, apoptosis, and tumorigenesis (3). siRNA is also used in therapeutic applications to identify drug targets and to characterize gene functions in vivo without the use of gene knockout mice (4). Formulation of siRNAs with compounds to promote transit across cell membranes is being developed to address the major challenge of cellular delivery of siRNAs (5). Several imaging modalities have been used for localized in vivo delivery of siRNA (6, 7).

Green fluorescence protein (GFP) is a reporter protein of 238 amino acids, and it emits a bright green fluorescence (λ_max_ = 509 nm) when illuminated with a blue light (λ_max_ = 395 nm) (8). Red fluorescent protein (RFP; excitation = 558 nm, emission = 583 nm) is another reporter protein of 28 kDa that shares ~25% sequence identity with GFP (9). GFP has a cylinder-like structure composed of eleven β-sheets slightly twisted around the central axis and a tripeptide (serine^65^-tyrosine^66^-glycine^67^) fluorophore attaching to the α-helix in the cylinder center (9, 10). As a tag or indicator, GFP is widely used to detect gene expression, protein trafficking, and cellular localization (11). Its fluorescence directly reflects the levels of gene expression or locations in subcellular compartments. Because GFP has no inherent localization of its own, fusion of GFP with functional proteins will typically result in the subcellular distribution pattern of the target protein (9). Thus, the fusion of GFP with host proteins is used to separate subcellular compartments in various cell organelles, including plasma membrane nucleus, endoplasmic reticulum, Golgi apparatus, secretary vesicles, mitochondria, peroxisomes, and phagosomes (12). The GFP/RFP reporter gene can be incorporated into recombinant plasmids, where it is directly linked to the transcriptional regulatory elements (11). Transfection of such recombinant plasmids into cells of interest allows for evaluation of promoter and enhancer activity. In combination with the RNAi technique, a GFP-specified siRNA (siGFP) can be used to generate animal models that are directly detectable with an optical microscope without the need for additional histological staining (13). For instance, 9L gliosarcoma cells can be transfected with the pcDNA3 (phGFP-S65T)-GFP/RFP plasmid to generate 9L-GFP/RFP glioma cells (13).

GFP-specified siRNA-crosslinked iron oxide nanoparticles (CLIO)-Cy5.5 (siGFP-CLIO-Cy5.5) is a magnetofluorescent nanoparticle used for multimodal imaging of the delivery and silencing of siGFP in tumors (6). This agent consists of four components: five siGFPs (22nt) to target GFP mRNA, three fluorescence probes (Cy5.5) for optical imaging, four myristoylated polyarginine peptides (MPAP) for mediating transportation to the cytoplasm, and an iron oxide nanoparticle core for enhancing magnetic resonance imaging (MRI) contrast and delivering siGFP to tumors. The siGFP is linked to magnetic nanoparticles by a stable thioether bond without compromising silencing efficiency. Cy5.5 is a cyanine dye consisting of two quaternized heteroaromatic bases (A and A’) joined by a polymethine chain with five carbons (14), which binds directly to the nanoparticles. This dye possesses high quantum yield, good chemical stability, easy conjugation, and high sensitivity (mole extinction coefficient, ~250,000 mol/cm) (15, 16). As a membrane translocation module, MPAP has a hydrophobic 14-carbon moiety of myristic acid (Myr, -C(=O)-(CH_2_)_12_-CH_3_) linked to a polyarginine peptide to generate Myr-Ala-(Arg)_7_-Cys-CONH_2_ (17). MPAP can cross the cellular membrane of live cells efficiently and target the cytoplasm without registered toxicity (17). The nanoparticle contains an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) that is caged by epichlorohydrin cross-linked dextran and functionalized with amine groups (CLIO-NH_2_) (18). They have a high magnetic susceptibility to induce a significant magnetization inside a magnetic field. This creates microscopic field gradients that diphase nearby protons and causes a shortening of T_2_ relaxation times (19). Enhanced permeability and retention effects in tumors and an increased fluid-phase endocytosis in tumor cells results in the accumulation of magnetic nanoparticles in the tumors (6). With the assistance of MPAP, sufficient siGFP can be delivered to the tumors. siGFP-CLIO-Cy5.5 allows for fine resolution (10–100 μm) and unlimited depth penetration of MRI with the high sensitivity (10^-9^–10^-17^ mol/L) and the short acquisition times of optical imaging (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO + cy5.5 + siGFP)+AND+synthesis%0D%0A)]

The synthesis of siGFP-CLIO-Cy5.5 was conducted in multiple steps (6). Initially, monocrystalline iron oxide (MION) was synthesized by neutralization of ferrous salts, ferric salts, and dextran with ammonium hydroxide, followed by ultrafiltration (20). The obtained MION was cross-linked in strong base with epichlorohydrin and then reacted with ammonia to produce CLIO-NH_2._ Next, N-hydroxysuccinimide ester of Cy5.5 was reacted with the CLIO-NH_2_ (21). The produced CLIO-Cy5.5 was conjugated with a heterobifunctional cross-linker, N-succinimidyl 3-(2-pyridyldithio)propionate (SPDP), via N-hydroxy succinimide ester. Then, Myr-Ala-(ARg)_7_-Cys-CONH_2_ MPAPs were attached to this linker via a sulfhydryl reactive pyridyl disulfide residue (pH 7). The produced CLIO(MPAP)-Cy5.5 was coupled with a m-maleimidobenzoyl-N-hydroxysuccinimide ester (MBS) cross-linker (pH 8.5). At the same time, commercial GFP siRNA duplex, a 22nt siRNA duplex directed against the sequence 5’-GCA AGC TGA CCC TGA AGT TC-3’ at nucleotides 122–141 of phGFP-S65T, was modified with a thiol moiety via a hexyl spacer (5’-S-S-(CH_2_)_6_-) for bioconjugation. Finally, the free thiol single-stranded RNA was reacted with the CLIO(MPAP)-Cy5.5 via the MBS cross-linker to produce siGFP-CLIO-Cy5.5. For the biodistribution studies, the MPAP peptide on the siGFP-CLIO-Cy5.5 was modified to contain an additional tyrosine at its carboxyl terminus for exchange with ^125^I (^125^I-labeled siGFP-CLIO-Cy5.5). The analysis results demonstrated that on average there were three Cy5.5, four MPAP, and five siGFP molecules per paramagnetic nanoparticles.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( CLIO + cy5.5 + siGFP)+AND+%22in+vitro%22)]

The uptake and silencing efficiency of siGFP-CLIO-Cy5.5 were measured in 9L-GFP (GFP-S65T) gliosarcoma cells with 9L-RFP (DsRed2) gliosarcoma cells as the control (6). The cells were incubated with siGFP-CLIO-Cy5.5 at different concentrations. The Cy5.5 fluorescence measured at 48 h after injection exhibited a linear dependence on the concentration of siGFP-CLIO-Cy5.5, which reflected increased uptake of siGFP-CLIO-Cy5.5 by the cells. The presence of MPAP membrane translocation peptides appeared to enhance cellular uptake of siGFP-CLIO-Cy5.5 substantially. The silencing efficiency in 9L-GFP cells was concentration-dependent, and the decrease in GFP fluorescence became significant at 48 h. In comparison, the fluorescence in 9L-RFP cells remained nearly the same as preincubation levels. This result was further confirmed with confocal microscopy, in which extensive cytoplasmic Cy5.5 fluorescence was found in both 9L-GFP cells and 9L-RFP cells after 48 h of incubation. siGFP-CLIO-Cy5.5 was found to be located in the perinuclear region as a result of sequestration by the RNA-induced silencing complex (RISC).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siGFP) +AND++rodentia)]

Biodistribution studies of siGFP-CLIO-Cy5.5 were conducted in mice (6). ^125^I-Labeled siGFP-CLIO-Cy5.5 at a dose of 10 mg Fe/kg (440 nmol siRNA/kg) was intravenously injected into mice (n = 3) that were bilaterally implanted with 9L-GFP and 9L-RFP tumors. Mice were euthanized 24 h after injection, and tissues were harvested for gamma counting. The distribution (percent injected dose (% ID)/g tissue) of ^125^I was 4.5 in the liver, 0.45 in the spleen, 0.22 in blood, 0.2 in 9L-GFP tumors, and 0.21 in 9L-RFP tumors. This was consistent with the accumulation and metabolic process found for iron oxide nanoparticles.

Medarova et al. studied the in vivo effect of siGFP-CLIO-Cy5.5 in tumors (6). Mice (n = 5) were bilaterally implanted with 9L-GFP and 9L-RFP tumors. The delivery of siGFP-CLIO-Cy5.5 was examined with MRI at 4.7 T; T_2_-weighted imaging was performed before and 24 h after injection of siGFP-CLIO-Cy5.5 at a dose of 10 mg Fe/kg (440 nmol siRNA/kg). The tumor appeared bright before injection and darkened significantly after injection. The delivery of siGFP-CLIO-Cy5.5 to the tumors was further confirmed ex vivo with MRI at 14 T and with near-infrared optical imaging measurement of Cy5.5 signal. The silencing efficiency of siGFP-CLIO-Cy5.5 was measured with in vivo optical imaging in the GFP and RFP channels before injection and 48 h after injection. GFP fluorescent signal in the 9L-GFP tumors was decreased 48 h after injection. The silencing effect was further confirmed with ex vivo optical imaging and confocal microscopy in the excised tumors. The confocal microscopic images of frozen tumor sections demonstrated that siGFP-CLIO-Cy5.5 accumulated in tumor-recruited macrophages. Quantitative reverse-transcription polymerase chain reaction was used to analyze the levels of Gfp mRNA in tumors. The level for mice treated with siGFP-CLIO-Cy5.5 was found to be 85 ± 2% lower than for mice treated with saline; these levels were 97 ± 1% lower than mice treated with mismatch siRNA.

Medarova et al. also examined the immunostimulatory and cytotoxic effects of siGFP-CLIO-Cy5.5 (6). No significant increase in the levels of serum interferon-α or inflammatory cytokines (interleukin-6) was found in mice treated with siGFP-CLIO-Cy5.5 compared with the levels of the parental unmodified magnetic nanoparticle (CLIO) or to non-treated controls. No elevated toxicity of siGFP-CLIO-Cy5.5 was found in treated mice compared to the controls by evaluation of serum aspartate aminotransferase and alanine aminotransferase levels. The apoptosis in tumors treated with siGFP-CLIO-Cy5.5 remained at the same levels as in tumors treated with CLIO.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siGFP) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siGFP) +AND+human)]

No publication is currently available.

## References

1 Chiu Y.L., Ali A., Chu C.Y., Cao H., Rana T.M. (2004). Visualizing a correlation between siRNA localization, cellular uptake, and RNAi in living cells. Chem Biol.
2 Dykxhoorn D.M., Novina C.D., Sharp P.A. (2003). Killing the messenger: short RNAs that silence gene expression. Nat Rev Mol Cell Biol.
3 Fuchs U., Borkhardt A. (2007). The application of siRNA technology to cancer biology discovery. Adv Cancer Res.
4 Tiscornia G., Singer O., Ikawa M., Verma I.M. (2003). A general method for gene knockdown in mice by using lentiviral vectors expressing small interfering RNA. Proc Natl Acad Sci U S A.
5 Mahmood Ur R., Ali I., Husnain T., Riazuddin S. (2008). RNA interference: The story of gene silencing in plants and humans. Biotechnol Adv.
6 Medarova Z., Pham W., Farrar C., Petkova V., Moore A. (2007). In vivo imaging of siRNA delivery and silencing in tumors. Nat Med.
7 Liu N., Ding H., Vanderheyden J.L., Zhu Z., Zhang Y. (2007). Radiolabeling small RNA with technetium-99m for visualizing cellular delivery and mouse biodistribution. Nucl Med Biol.
8 Chalfie M., Tu Y., Euskirchen G., Ward W.W., Prasher D.C. (1994). Green fluorescent protein as a marker for gene expression. Science.
9 Day R.N., Periasamy A., Schaufele F. (2001). Fluorescence resonance energy transfer microscopy of localized protein interactions in the living cell nucleus. Methods.
10 Schmid J.A., Neumeier H. (2005). Evolutions in science triggered by green fluorescent protein (GFP). Chembiochem.
11 Kar-Roy A., Dong W., Michael N., Li Y. (2000). Green fluorescence protein as a transcriptional reporter for the long terminal repeats of the human immunodeficiency virus type 1. J Virol Methods.
12 Greenbaum L., Schwartz D., Malik Z. (2002). Spectrally resolved microscopy of GFP trafficking. J Histochem Cytochem.
13 Moore A., Marecos E., Simonova M., Weissleder R., Bogdanov A. (1998). Novel gliosarcoma cell line expressing green fluorescent protein: A model for quantitative assessment of angiogenesis. Microvasc Res.
14 Ernst L.A., Gupta R.K., Mujumdar R.B., Waggoner A.S. (1989). Cyanine dye labeling reagents for sulfhydryl groups. Cytometry.
15 Lin Y., Weissleder R., Tung C.H. (2002). Novel near-infrared cyanine fluorochromes: synthesis, properties, and bioconjugation. Bioconjug Chem.
16 Ballou B., Fisher G.W., Hakala T.R., Farkas D.L. (1997). Tumor detection and visualization using cyanine fluorochrome-labeled antibodies. Biotechnol Prog.
17 Pham W., Zhao B.Q., Lo E.H., Medarova Z., Rosen B., Moore A. (2005). Crossing the blood-brain barrier: a potential application of myristoylated polyarginine for in vivo neuroimaging. Neuroimage.
18 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
19 Bulte J.W., Brooks R.A., Moskowitz B.M., Bryant L.H., Frank J.A. (1998). T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment. Acad Radiol.
20 Wunderbaldinger P., Josephson L., Weissleder R. (2002). Crosslinked iron oxides (CLIO): a new platform for the development of targeted MR contrast agents. Acad Radiol.
21 Montet X., Montet-Abou K., Reynolds F., Weissleder R., Josephson L. (2006). Nanoparticle imaging of integrins on tumor cells. Neoplasia.